# ^123^I-Labeled (S)-2-(3-((S)-1-carboxy-5-(3-(4-iodophenyl) ureido)pentyl)ureido)pentanedoic acid

Chemical name: | ^123^I-Labeled (S)-2-(3-((S)-1-carboxy-5-(3-(4-iodophenyl) ureido)pentyl)ureido)pentanedoic acid
Abbreviated name: | [^123^I]MIP-1095
Synonym:
Agent Category: | Compound
Target: | Prostate-specific membrane antigen (PSMA) or glutamate carboxypeptidase II (GCP II) or folate hydrolase or N-acetylated-α-linked-acidic-dipeptidase (NAALADase)
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography/computed tomography (SPECT/CT)
Source of signal / contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for additional information regarding [^123^I]MIP1095 in PubChem (http://pubchem.ncbi.nlm.nih.gov/deposit/deposit.cgi?s=submgr&ss=submarch&mid=265419). Click on protein (http://www.ncbi.nlm.nih.gov/protein/Q04609.1?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_153696.2?ordinalpos=2&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=2346&log$=genesensor5&logdbfrom=nuccore) for additional information regarding the human PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MIP+1072)]

The prostate-specific membrane antigen (PSMA), a membrane-bound glycoprotein that possesses different peptidase activities (see Table above), is expressed mainly in the prostate epithelium. Because of its overexpression in primary, metastatic or hormone-refractory prostate and other cancers, including the neovasculature of solid tumors, this antigen is considered to be a cancer marker and a good target for imaging agents and therapy (1). Hence, PSMA has been targeted in several clinical trials (http://clinicaltrials.gov/ct2/results?term=PSMA) that have been approved by the United States Food and Drug Administration (FDA) for the treatment of prostate cancer. In addition, capromab pendetide, a commercially available monoclonal antibody (MAb) that binds to the intracellular domain of the PSMA and was approved by the FDA for the diagnostic imaging of prostate cancer (http://www.prostascintimaging.com./hcp/prostascint/), has limited use because the MAb binds primarily to necrotic parts of the tumor and may not detect any viable malignant tumor cells (2). Investigators have also developed and evaluated MAbs directed against the extracellular domains of PSMA, and after preclinical studies they reported that these MAbs could be of potential use in the detection and treatment of PSMA-positive cancers (3-5). However, results obtained from a phase I clinical trial to evaluate the use of ^111^In-labeled/unlabeled J591 MAb mixture to detect and target the PSMA-positive vasculature of progressive solid tumors in patients with breast, colon, liver, or kidney cancers showed that, although the antibody was well tolerated, selectively targeted a variety of solid tumors, but it did not yield any positive therapeutic response(s) (6). The investigators concluded that this was probably because the large molecular size of the MAb was a hindrance to its complete penetration into the tumors. In addition, therapeutic MAbs have poor pharmacokinetic profiles in normal tissues because they have an extended circulation period compared with the small molecule drugs.

Radiolabeled small molecule drugs have an advantage over MAbs because they are inexpensive to produce, can easily penetrate solid tumors, and, due to their pharmacokinetic properties, are superior for use in the detection (by imaging techniques) and therapy of cancerous tumors. On the basis of the facts presented above, a series of small-molecule inhibitors of PSMA were recently synthesized for possible use in conjunction with single-photon emission computed tomography/computed tomography (SPECT/CT) for the detection and staging of prostate cancer (7). Two of these compounds, (S)-2-(3-((S)-1-carboxy-5-(3-(4-iodophenyl)ureido)pentyl)ureido)pentanedoic acid (MIP-1095) and (S)-2-(3-((S)-1-carboxy-5-(3-(4-iodobenzylamino)pentyl)ureido)pentanedoic acid (MIP-1072), were labeled with ^123^I by Hillier et al. for evaluation as molecular imaging agents to detect prostate cancer in a mouse model (8). This chapter describes the studies performed with [^123^I]MIP-1095 under in vitro conditions and its biodistribution in mice bearing LNCaP (derived from human metastatic prostate carcinoma; expresses PSMA) and PC (developed from the bone marrow of a patient with secondary myelodisplastic syndrome; does not express PSMA; for further details regarding this cell line please see (9)) cell xenograft tumors. Studies performed with [^123^I]MIP-1072 are presented in a separate chapter in MICAD (www.micad.nih.gov) (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP-1072+synthesis)]

The synthesis and radioiodination of MIP-1095 was performed as described by Maresca et al. (7). The radiochemical yield was 50–70%, and purity of the labeled compound was reported to be >90%. Identity of the radioiodinated compound was confirmed with reverse-phase high-performance liquid chromatography (RP-HPLC) by co-injecting the tracer with its corresponding unlabeled compound. Specific activity of the iodinated compound was reported to be ≥148 MBq/μmol (≥4 Ci/μmol). [^123^I]MIP-1095 was reported to be stable at 40°C for at least 48 h as determined with RP-HPLC (7).

For comparative studies, [^123^I]MIP-1072 was also synthesized as above and had a similar yield, radiochemical purity, and specific activity as [^123^I]MIP-1095 (8). In addition, capromab pendetide was labeled with ^111^In to compare its biodistribution with [^123^I]MIP-1095 in xenograft mice. The specific activity of the ^111^In-labeled MAb was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+in+vitro)]

Hillier et al. used LNCaP cells to determine the in vitro characteristics of [^123^I]MIP-1095 (8). Using [^3^H]-N-acetyl-aspartyl-glutamate as a substrate for N-acetylated-α-linked-acidic-dipeptidase (NAALADase), the inhibition constant (K_i_) of MIP-1095 was determined to be 0.24 ± 0.14 nmol/L (8). The dissociation constant (K_d_) and maximal binding (B_max_) of [^123^I]MIP-1072 for PSMA expressed on the LNCaP cells were reported to be 0.81 ± 0.39 nmol/L and 1,490 ± 60 fmol/10^6^ cells (0.9 × 10^6^ sites/cell), respectively. In addition, similar to [^123^I]MIP-1072, [^123^I]MIP-1095 was also internalized by the LNCaP cells (8). The K_i_ and K_d_ values of [^123^I]MIP-1072 were higher than those obtained with [^123^I]MIP-1095 (K_i_ and K_d_ were 4.6 ± 1.6 nmol/L and 3.8 ± 1.3 nmol/L, respectively); as expected, the B_max_ values obtained with both compounds were similar. The binding of [^123^I]MIP-1095 to LNCaP cells was shown to be inhibited (>95%) by 2-(phosphonomethyl)-pentanedioic acid (PMPA), a NAALADase inhibitor, as observed with [^123^I]MIP-1072.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+rodentia)]

The biodistribution of [^123^I]MIP-1095 was investigated in male NCr-nu/nu mice bearing LNCaP cell xenograft tumors (8). The animals were injected with the radiochemical through the tail vein and euthanized at predetermined time points (n = 5 mice/time point) varying from 15 min to 24 h after the treatment. The tumors and other important tissues were then collected from the animals to determine tracer uptake (expressed as percent injected dose/gram tissue (% ID/g)). By 24 h after treatment, the non-target tissues, including blood, had very low accumulation of radioactivity. At this time point a high amount of label was present in the tumor (29.10 ± 15.10% ID/g) followed by the kidneys (27.00 ± 26.20% ID/g; these organs have a high PSMA content). The tumors had a maximum amount of accumulated tracer (34.30 ± 12.70% ID/g) at 4 h after the injection, and the uptake peaked in the kidneys (88.70 ± 23.80% ID/g) at 2 h after treatment. By comparison, the accumulation of [^123^I]MIP-1072 in the tumor and kidneys at 24 h was 5.03 ± 1.35% ID/g and 1.10 ± 0.60% ID/g, respectively. Unlike [^123^I]MIP-1095, the label from ^111^In-labeled capromab pendetide was present at higher levels in all target and non-target organs even 72 h after the injection. The tumor/blood and tumor/skeletal muscle ratios were 174 and 304, 411 and 64.5 (at 24 h after the injection), and 2.92 and 41.2 (at 72 h after the injection) for [^123^I]MIP-1072, [^123^I]MIP-1095, and ^111^In-labeled capromab pendetide, respectively (8). The investigators also noted that the clearance of [^123^I]MIP-1095 from the tumors was slower than that of [^123^I]MIP-1072 (P < 0.05), and there was no significant difference (P > 0.06) in the tumor levels of [^123^I]MIP-1095 between 1 h and 24 h after injection of the tracer. In general, compared with [^123^I]MIP-1072, a slower (P < 0.05) clearance of [^123^I]MIP-1095 was noted from the non-target tissues between 1 h and 8 h after the radiotracer injection. Although the brain contains a high level of NAALADase activity (11), little uptake of either [^123^I]MIP-1095 or [^123^I]MIP-1072 was observed in this organ, indicating that these radiochemicals did not cross the blood–brain barrier.

To investigate the in vivo binding specificity of [^123^I]MIP-1095 in mice bearing LNCaP tumors (n = 5 animals), the animals were injected with the radiochemical in the presence of excess PMPA (50 mg/kg animal body weight) and euthanized 2 h later (8). Under these conditions the accumulation of [^123^I]MIP-1095 in the tumors and kidneys was reported to be almost completely blocked. This indicated that accumulation of the radiochemical in these tissues was mediated by the specific binding of [^123^I]MIP-1095 to PSMA.

Similar to the biodistribution studies, SPECT/CT imaging of mice bearing LNCaP (PSMA+ve), PC (PSMA-ve), or PC3 PIP (PC3 cells transfected with the PSMA gene) cell xenograft tumors 4 h after injection with [^123^I]MIP-1095 showed that the label accumulated primarily in the PSMA+ve tumors and kidneys of the animals. This indicated that the uptake of [^123^I]MIP-1095 was specific due to the expression of PSMA on the cells and not as a consequence of blood flow or permeability differences between tumors derived from the different cell lines.

From these studies, the investigators concluded that both [^123^I]MIP-1095 and [^123^I]MIP-1072 could be developed for imaging, therapy (by attaching an appropriate nuclide to the molecules), and monitoring of prostate cancer in humans (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+MIP+1072+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

This work was supported by National Institutes of Health grants R43 EB004253, U24 CA92871, and R01 CA134675.

## References

1 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
2 Troyer J.K., Beckett M.L., Wright G.L. (1997). Location of prostate-specific membrane antigen in the LNCaP prostate carcinoma cell line. Prostate.
3 Smith-Jones P.M., Vallabhajosula S., Navarro V., Bastidas D., Goldsmith S.J., Bander N.H. (2003). Radiolabeled monoclonal antibodies specific to the extracellular domain of prostate-specific membrane antigen: preclinical studies in nude mice bearing LNCaP human prostate tumor. J Nucl Med.
4 Vallabhajosula S., Goldsmith S.J., Kostakoglu L., Milowsky M.I., Nanus D.M., Bander N.H. (2005). Radioimmunotherapy of prostate cancer using 90Y- and 177Lu-labeled J591 monoclonal antibodies: effect of multiple treatments on myelotoxicity. Clin Cancer Res.
5 Milowsky M.I., Nanus D.M., Kostakoglu L., Sheehan C.E., Vallabhajosula S., Goldsmith S.J., Ross J.S., Bander N.H. (2007). Vascular targeted therapy with anti-prostate-specific membrane antigen monoclonal antibody J591 in advanced solid tumors. J Clin Oncol.
6 Morris M.J., Pandit-Taskar N., Divgi C.R., Bender S., O'Donoghue J.A., Nacca A., Smith-Jones P., Schwartz L., Slovin S., Finn R., Larson S., Scher H.I. (2007). Phase I evaluation of J591 as a vascular targeting agent in progressive solid tumors. Clin Cancer Res.
7 Maresca K.P., Hillier S.M., Femia F.J., Keith D., Barone C., Joyal J.L., Zimmerman C.N., Kozikowski A.P., Barrett J.A., Eckelman W.C., Babich J.W. (2009). A series of halogenated heterodimeric inhibitors of prostate specific membrane antigen (PSMA) as radiolabeled probes for targeting prostate cancer. J Med Chem.
8 Hillier S.M., Maresca K.P., Femia F.J., Marquis J.C., Foss C.A., Nguyen N., Zimmerman C.N., Barrett J.A., Eckelman W.C., Pomper M.G., Joyal J.L., Babich J.W. (2009). Preclinical evaluation of novel glutamate-urea-lysine analogues that target prostate-specific membrane antigen as molecular imaging pharmaceuticals for prostate cancer. Cancer Res.
9 Serrero G., Zhou J., Mills D., LePak N. (1991). Decreased transforming growth factor-beta response and binding in insulin-independent teratoma-derived cell lines with increased tumorigenic properties. J Cell Physiol.
10 Chopra, A., [123I]-Labeled (S)-2-(3-((S)-1-carboxy-5-(4-iodobenzylamino) ureido)pentyl)ureido)pentanedoic acid [123I]MIP-1072. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Tiffany C.W., Lapidus R.G., Merion A., Calvin D.C., Slusher B.S. (1999). Characterization of the enzymatic activity of PSM: comparison with brain NAALADase. Prostate.